# Tri-methoxy-tris-pyrazolyl-^99m^Tc-(CO)_3_

Chemical name: | Tri-methoxy-tris-pyrazolyl-^99m^Tc-(CO)_3_ | [image]
Abbreviated name: | ^99m^Tc-TMEOP | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Non-targeted | [image]
Target Category: | Non-targeted | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) or planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^99m^Tc-TMEOP, ^99m^Tc-sestamibi, and ^99m^Tc-tetrofosmin (1, 2).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=myocardial%20perfusion%20imaging%20and%20radiotracers)]

Tri-methoxy-tris-pyrazolyl-^99m^Tc-(CO)_3_, abbreviated as ^99m^Tc-TMEOP, is a radiotracer synthesized by Goethals et al. for myocardial perfusion imaging with single-photon emission computed tomography (SPECT) or planar imaging (1).

Myocardial perfusion imaging is widely used to assess the blood flow to myocardium during periods of exercise (or stress) and rest (3-5). To precisely assess the blood flow, diverse compounds labeled with various radionuclides have been synthesized and tested in animals and in the clinic (2, 6). Basically, two major issues have to be considered when designing a radiotracer for perfusion imaging. The first issues to be considered are the flow-extraction rate and heart uptake (1, 2). The first-pass myocardial extraction fraction and heart uptake should be high enough to produce a strong signal for myocardial imaging. Both parameters are also essential to obtain high heart/liver, heart/lung, and heart/blood signal ratios at the early time point after injection of the radiotracers. Currently, most radiotracers are labeled with ^99m^Tc, have a first-pass extraction fraction from 29% to 90%, show a heart uptake from 1% to 3% injected dose (ID), and display a myocardial signal proportional to the regional myocardial blood flow (2). However, some tracers can underestimate the blood flow in the high flow ranges (>2 mL.g−^1^·min−^1^) and overestimate the blood flow in the low flow ranges (<0.2 mL.g−^1^·min−^1^) (2, 4). The second issues to be considered are the liver uptake and clearance, which can significantly influence the diagnostic specificity of myocardial ischemia. Unfortunately, most ^99m^Tc-labeled radiotracers suffer from high liver uptake with slow clearance, which leads to a high percentage of false-positive or negative results for myocardial ischemia, especially for ischemia in the inferior wall of heart (1). Stimulating patients by eating fatty food before imaging can reduce the liver signal, but the results can vary significantly between individual patients. An optimal radiotracer should have less liver uptake but fast clearance from liver.

To overcome the problem of high liver uptake, Goethals et al. synthesized a new radiotracer, ^99m^Tc-TMEOP, based on tri-carbonyl chemistry (1). TMEOP is a neutral and tridentate nitrogen donor chelator that forms a moderately lipophilic cationic complex upon reaction with the organometallic precursor fac-[^99m^Tc(OH)_2_(CO)_3_]^+^. The investigators evaluated the in vitro properties and in vivo pharmacokinetics of ^99m^Tc-TMEOP and compared them with the data obtained with ^99m^Tc-sestamibi (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm) and ^99m^Tc-tetrofosmin (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm), two radiotracers approved for clinical use by the United States Food and Drug Administration (1). The results showed that ^99m^Tc-TMEOP uptake in the heart was between those of ^99m^Tc-sestamibi and ^99m^Tc-tetrofosmin, but ^99m^Tc-TMEOP exhibited a faster liver washout (1). This chapter summarizes the data obtained with ^99m^Tc-TMEOP.

### Related Resource Links:

Clinical trials of myocardial perfusion imaging (http://clinicaltrials.gov/ct2/results?term=myocardial+perfusion+imaging)

Myocardial perfusion imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=myocardial%20perfusion%20imaging%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861278)]

The synthesis of ^99m^Tc-TMEOP was achieved by heating the solution of [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ (pH 4) and TMEOP ligand in ethanol for 45 min at 100°C (1). After cooling, the pH was adjusted to 7.4. ^99m^Tc-Sestamibi and ^99m^Tc-tetrofosmin were prepared according to the manufacturers’ instructions. The log P value of ^99m^Tc-TMEOP was determined with n-octanol phosphate-buffered saline (PBS) system (pH 7.4) by multiple back-extraction method.

The complex ^99m^Tc-TMEOP was obtained in a quantitative yield with a high radiochemical purity (>98%). The chemical identity of ^99m^Tc-TMEOP was established by comparing its radiochromatogram with the UV-vis trace of the Re surrogate. ^99m^Tc-TMEOP was moderately lipophilic with a log P value of 0.61 ± 0.04, which was at the low end of the range considered adequate to have significant heart uptake and favorable liver clearance kinetics (1). The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861278)]

The in vitro stability of ^99m^Tc-TMEOP was studied after incubation at 37°C with PBS (pH 7.4) and with human serum, respectively (1). ^99m^Tc-TMEOP was stable and did not undergo any transformation, including reoxidation to pertechnetate, even after 24 h of incubation in PBS and after 2 h of incubation in human serum. Also, ^99m^Tc-TMEOP did not show binding to any human serum proteins.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861278)]

The in vivo stability of ^99m^Tc-TMEOP was determined after injection of ^99m^Tc-TMEOP (7–20 MBq (0.19–0.54 mCi)) into Sprague-Dawley rats (n = 4) (1). Analysis of ex vivo tissues showed that the compound remained unchanged in all tissues at 1 h and 2 h after injection.

Pharmacokinetics was performed in healthy male Wistar rats (n = 18) (1). Each animal received an intravenous injection of 250 MBq (6.76 mCi) ^99m^Tc-TMEOP, ^99m^Tc-sestamibi, or ^99m^Tc-tetrofosmin (n = 6 rats per tracer). Dynamic planar imaging was carried out for 1 h with a dual-headed gamma camera. ^99m^Tc-TMEOP showed a significantly higher heart uptake than ^99m^Tc-tetrofosmin (P < 0.05) starting from 5 min after injection and a heart uptake comparable to ^99m^Tc-sestamibi (P > 0.05) (Table 1). In the liver, the uptake of ^99m^Tc-TMEOP was significantly lower than that of ^99m^Tc-tetrofosmin (P < 0.05 between 16.5 min and 40.5 min) and ^99m^Tc-sestamibi (P < 0.05 from 16 min). Thus, the heart/liver ratio was significantly higher for ^99m^Tc-TMEOP than for ^99m^Tc-tetrofosmin (from 5 min) and ^99m^Tc-sestamibi (from 16.5 min). However, there was no difference in the lung uptake or heart/lung ratio among the three radiotracers, although ^99m^Tc-TMEOP demonstrated the lowest initial pulmonary uptake.

Table 1: Total cardiac uptake (percentage of injected activity).

Radiotracer | 20 min | 40 min | 60 min | 120 min
^99m^Tc-TMEOP | 1.34 ± 0.09 | 1.31 ± 0.08 | 1.28 ± 0.06 | 1.29 ± 0.16
^99m^Tc-sestamibi | 1.42 ± 0.11 | 1.39 ± 0.11 | 1.36 ± 0.11 | 1.26 ± 0.10
^99m^Tc-tetrofosmin | 1.21 ± 0.07 | 1.20 ± 0.06 | 1.16 ± 0.05 | 1.11 ± 0.09

Cardiac pinhole-gated SPECT imaging was performed at 40 min after injection (n = 6 rats) (1). The quality of the left ventricular perfusion images obtained with ^99m^Tc-TMEOP was comparable to the quality of images obtained with ^99m^Tc-sestamibi and ^99m^Tc-tetrofosmin. All images showed homogeneous perfusion in the left ventricular wall. The heart/liver ratio was two times higher for ^99m^Tc-TMEOP than for ^99m^Tc-sestamibi and ^99m^Tc-tetrofosmin.

Table 2: Pinhole-gated SPECT comparison.

Radiotracer | Heart/liver ratio | End-diastolic volume (ml) | End-systolic volume (ml) | Ejection fraction
^99m^Tc-TMEOP | 6.98 ± 1. 66 | 0.39 ± 0.06 | 0.12 ± 0.03 | 70.7 ± 3.5
^99m^Tc-sestamibi | 2.48 ± 0.30 | 0.39 ± 0.04 | 0.11 ± 0.02 | 72 ± 2.6
^99m^Tc-tetrofosmin | 2.66 ± 0.40 | 0.38 ± 0.05 | 0.11 ± 0.03 | 70 ± 2.6

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21861278)]

No references are currently available.

## References

1 Goethals L.R., et al. (2011). Rapid hepatic clearance of 99mTc-TMEOP: a new candidate for myocardial perfusion imaging. Contrast Media Mol Imaging.
2 Lin X., et al. (2012). Development of radiolabeled compounds for myocardial perfusion imaging. Curr Pharm Des.
3 Anagnostopoulos C., et al. (2003). Procedure guidelines for radionuclide myocardial perfusion imaging. Nucl Med Commun.
4 Clark A.N., Beller G.A. (2005). The present role of nuclear cardiology in clinical practice. Q J Nucl Med Mol Imaging.
5 Gimelli A., et al. (2009). Stress/Rest Myocardial Perfusion Abnormalities by Gated SPECT: Still the Best Predictor of Cardiac Events in Stable Ischemic Heart Disease. J Nucl Med.
6 Sciagra R., Leoncini M. (2005). Gated single-photon emission computed tomography. The present-day ''one-stop-shop'' for cardiac imaging. Q J Nucl Med Mol Imaging.